# 6,7-Dimethoxy-2-{3-[4-[^11^C]methoxy-3,4-dihydro-2H-naphthalen-(1E)-ylidene]-propyl}-1,2,3,4-tetrahydro-isoquinoline

Chemical name: | 6,7-Dimethoxy-2-{3-[4-[^11^C]methoxy-3,4-dihydro-2H-naphthalen-(1E)-ylidene]-propyl}1,2,3,4-tetrahydro-isoquinoline
Abbreviated name: | [^11^C]6
Synonym:
Agent category: | Compound
Target: | P-glycoprotein multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp)]

One of the mechanisms of tumor cells to escape the cytotoxic effects of chemotherapeutic agents, such as adriamycin, vinca alkaloids, epipodophyllotoxins, actinomycin D, and paclitaxel, is to limit their presence inside the cells by way of a multidrug resistance (MDR-1) protein (1, 2). The MDR-1 gene encodes a transmembrane P-glycoprotein (P-gp) as an ATP-dependent multidrug transporter that is capable of actively pumping a variety of agents out of the cells. Injection of unlabeled efflux pump substrates increases the retention of the radioactivity in the tumor by blocking the efflux rather than reducing radioactivity uptake as seen with receptor-binding radiotracer blocking studies. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood–brain barrier (BBB) (4, 5). Calcium channel blockers (such as verapamil), cyclosporine (CsA, P-gp inhibitor) and CsA's non-immunosuppressive analog PSC 833 (other mechanism) are MDR modulators that inhibit the transport of P-gp substrates out of the cells (6, 7).

^99m^Tc-Sestamibi (MIBI) has been approved by the United States Food and Drug Administration as a myocardial perfusion imaging agent for use with single-photon emission computed tomography to assess the risk of future cardiac events (8). It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers (8-10). MIBI is a substrate for P-gp (4, 11). 6,7-Dimethoxy-2-{3-[4-methoxy-3,4-dihydro-2H-naphthalen-(1E)-ylidene]-propyl}-1,2,3,4-tetrahydro-isoquinoline (compound 6) is a P-gp inhibitor (12). 6,7-Dimethoxy-2-{3-[4-[^11^C]methoxy-3,4-dihydro-2H-naphthalen-(1E)-ylidene]-propyl}-1,2,3,4-tetrahydro-isoquinoline ([^11^C]6) is being developed as a positron emission tomography (PET) agent for the non-invasive study of the P-gp function and MDR in tumors and normal tissues (13).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D) (P-glycoprotein)
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D) (P-glycoprotein)
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20synthesis)]

[^11^C]6 was synthesized by reaction of the desmethyl precursor with [^11^C]methyl iodide for 4 min at 80°C (13). The radiochemical purity of purified [^11^C]6 was >98% with a specific activity of >100 GBq/µmol (2.7 Ci/µmol) at the end of synthesis. The total synthesis time was 45 min with a radiochemical yield of ~30%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20in%20vitro)]

Colabufo et al. (12) showed that compound 6 (5 µM) increased the intracellular uptake of doxorubicin in MCF7/adr cells by 4.7-fold and potentiated the anti-proliferation effect of doxorubicin (5 µM) from 5% to 95%. Compound 6 did not activate ATPase of the Caco-2 monolayer. Therefore, compound 6 was classified as a P-gp inhibitor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20rodentia)]

van Waarde et al. (13) performed ex vivo biodistribution studies with ~12 MBq (0.32 mCi) [^11^C]6 in normal rats (n = 4) at 60 min after injection. The accumulation of radioactivity expressed as standard uptake value (SUV) in various brain regions was 0.45–0.69. Pretreatment with compound 6 reduced the accumulation into the various brain regions by 30–40% (P < 0.05). Significant reduction (P < 0.05) was also observed in the colon (60%), duodenum (67%), ileum (53%), and spleen (35%). Significant enhancement (P < 0.05) was observed in the heart (42%) and lung (60%). The peripheral organ with the highest SUV was the pancreas (4.02), followed by the duodenum (3.06), spleen (2.66), ileum (1.94), and colon (1.85).

PET imaging showed an initial high accumulation of [^11^C]6 in the brains of rats at 0.5 min after injection, followed by a gradual washout. The brain was clearly visualized. Pretreatment with compound 6 (15 mg/kg) resulted in a 23% decrease in brain radioactivity at 56 min after [^11^C]6 injection. The brain SUV was 0.88 ± 0.04 for the control rats and 0.68 ± 0.03 for the rats treated with compound 6 (P < 0.01). Logan plot analysis with arterial input showed that compound 6 treatment decreased the cerebral distribution volume from 2.35 ± 0.11 to 1.65 ± 0.03 (P < 0.005) and the influx rate constant from 0.90 ± 0.08 to 0.45 ± 0.45.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28nonhuman%20primate%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28%20human%29)]

No publications are currently available.

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Olszowska M., Kostkiewicz M., Tracz W., Przewlocki T. (2003). Assessment of myocardial perfusion in patients with coronary artery disease. Comparison of myocardial contrast echocardiography and 99mTc MIBI single photon emission computed tomography. Int J Cardiol.
9 Benard F., Romsa J., Hustinx R. (2003). Imaging gliomas with positron emission tomography and single-photon emission computed tomography. Semin Nucl Med.
10 Peng N.J., Chang H.T., Tsay D.G., Liu R.S. (2003). Technetium-99m-sestamibi scintimammography to detect breast cancer in patients with paraffinomas or siliconomas after breast augmentation. Cancer Biother Radiopharm.
11 Piwnica-Worms D., Kronauge J.F., Holman B.L., Lister-James J., Davison A., Jones A.G. (1988). Hexakis(carbomethoxyisopropylisonitrile) technetium(I), a new myocardial perfusion imaging agent: binding characteristics in cultured chick heart cells. J Nucl Med.
12 Colabufo N.A., Berardi F., Cantore M., Perrone M.G., Contino M., Inglese C., Niso M., Perrone R., Azzariti A., Simone G.M., Porcelli L., Paradiso A. (2008). Small P-gp modulating molecules: SAR studies on tetrahydroisoquinoline derivatives. Bioorg Med Chem.
13 van Waarde A., Ramakrishnan N.K., Rybczynska A.A., Elsinga P.H., Berardi F., de Jong J.R., Kwizera C., Perrone R., Cantore M., Sijbesma J.W., Dierckx R.A., Colabufo N.A. (2009). Synthesis and preclinical evaluation of novel PET probes for P-glycoprotein function and expression. J Med Chem.